# 2,2,3,3-Tetramethylcyclopropanecarboxylic acid [3-(2-[^11^C]methoxyethyl)-4,5-dimethyl-3H-thiazol-(2Z)-ylidene]amide

Chemical name: | 2,2,3,3-Tetramethylcyclopropanecarboxylic acid [3-(2-[^11^C]methoxyethyl)-4,5-dimethyl-3H-thiazol-(2Z)-ylidene]amide
Abbreviated name: | [^11^C]A-836339
Synonym:
Agent category: | Compound
Target: | Cannabinoid CB2 receptors
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 receptors are expressed abundantly in neuronal terminals in the central nervous system (CNS) and in some peripheral tissues to inhibit neurotransmitter release. CB1 receptors are found predominately in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. CB2 receptors are present mainly on immune cells in the blood and peripheral tissues (the spleen) to modulate cytokine release (3). However, CB2 receptors have been found in the CNS tissues (neurons and glial cells) at very low levels (4). Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 receptors have been demonstrated to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 receptor function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (5-7). Upregulation of CB2 receptors in the brain is associated with neuroinflammation in disorders such as Alzheimer’s disease (AD), multiple sclerosis, encephalitis, and Down’s syndrome (8). CB2 receptors are also involved in inflammation associated with pain, osteoporosis, cancer, and liver diseases (9).

Δ9-Tetrahydrocannabinol (THC) is a major active cannabinoid found in marijuana, and it activates CB1 receptors (10). Various radioligands have been developed for imaging of CB1 receptors (11). However, only a few CB2 radioligands have been evaluated in animals as potential positron emission tomography (12) tracers (13-17). 2,2,3,3-Tetramethylcyclopropanecarboxylic acid [3-(2-[^11^C]methoxyethyl)-4,5-dimethyl-3H-thiazol-(2Z)-ylidene]amide ([^11^C]A-836339) has been evaluated for use as a CB2 radioligand for brain imaging of neuroinflammation and AD (18). A-836339 is a selective CB2 agonist with high binding (inhibition constant (K_i_), 0.64 nM) (19).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=(CB2%20OR%20CB1)+AND+micad%5Bbook%5D)
- Gene information in NCBI (CB2 receptors (http://www.ncbi.nlm.nih.gov/gene/1269))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/605051)
- Clinical trials (CB2 (http://www.clinicaltrials.gov/ct2/results?term=CB2))
- Drug information in FDA (CB2 (http://google2.fda.gov/search?q=CB2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339%20and%20synthesis)]

Horti et al. (18) reported the synthesis of [^11^C]A-836339 by reaction of the O-desmethyl precursor with [^11^C]methyl triflate for 5 min in the presence of potassium hydroxide in dimethylformamide. The average radiochemical yield was 26 ± 2% (non–decay-corrected) at the end of synthesis (EOS), with a total synthesis time of 40 min from the end of bombardment. Specific radioactivity was 304 ± 62 GBq/μmol (8.2 ± 1.7 Ci/μmol; n = 7) at EOS with a radiochemical purity of >99% after purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339%20and%20in%20vitro)]

Yao et al. (19) reported that A-836339 had K_i_ values of 0.64 nM and 270 nM for human CB2 and CB1, respectively. A-836339 exhibited K_i_ values of 0.76 nM and 143 nM for rat CB2 and CB1, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339%20and%20rodentia)]

Horti et al. (18) performed ex vivo biodistribution studies of [^11^C]A-836339 in normal mice (n = 3/group) at 30, 60, and 90 min after injection. The brain accumulation of radioactivity (0.3% injected dose/gram (ID/g)) at 30 min after injection was lower than that of the liver (4.9% ID/g), kidney (2.2% ID/g), intestine (1.5% ID/g), spleen (1.3% ID/g), and heart (0.7% ID/g). The selective CB2 antagonist AM630 (3 mg/kg, intravenous) significantly (P < 0.05) blocked radioactivity in the spleen when administered 30 min before injection of [^11^C]A-836339 in mice but had little effect on the binding in all other organs including the brain. Mice treated with lipopolysaccharide (LPS) for 5 days exhibited increased accumulation of [^11^C]A-836339 in the brainstem (+110%), hippocampus (+90%), cerebellum (+80%), and cortex (+70%) as compared with the control mice (P < 0.05). AM630 significantly (P < 0.05) reduced binding in the brainstem and hippocampus in the LPS-treated mice. Blocking experiments with AM630 showed little effect on the accumulation in the whole brain in control mice, whereas binding was reduced by 78% (P < 0.05) in the whole brain of LPS-treated mice.

PET imaging showed that the radioactivity in the whole brain of LPS-treated mice peaked (standard uptake value (SUV) = 2.3) at 3 min after [^11^C]A-836339 injection with washout. The cerebral SUV of the control mice was 0.5 at 3 min after injection with little washout. In a mouse model of AD (APPswe/PS1dE9 bigenic mice), [^11^C]A-836339 showed 29%–36% specific binding (AM630 blocking) in the cerebellum, brainstem, and cortex. The authors concluded that there is a need to develop tracers for CB2 PET imaging with lower lipophilicity and greater specific binding than [^11^C]A-836339.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20A-836339%20and%20human)]

No publication is currently available.

## NIH Support

MH079017

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee, R.G., Pharmacological actions of cannabinoids. Handb Exp Pharmacol, 2005(168): p. 1-51.
4 Onaivi E.S., Ishiguro H., Gong J.P., Patel S., Perchuk A., Meozzi P.A., Myers L., Mora Z., Tagliaferro P., Gardner E., Brusco A., Akinshola B.E., Liu Q.R., Hope B., Iwasaki S., Arinami T., Teasenfitz L., Uhl G.R. (2006). Discovery of the presence and functional expression of cannabinoid CB2 receptors in brain. Ann N Y Acad Sci.
5 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
6 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
7 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
8 Benito C., Tolon R.M., Pazos M.R., Nunez E., Castillo A.I., Romero J. (2008). Cannabinoid CB2 receptors in human brain inflammation. Br J Pharmacol.
9 Pertwee R.G. (2009). Emerging strategies for exploiting cannabinoid receptor agonists as medicines. Br J Pharmacol.
10 Martin B.R. (1986). Cellular effects of cannabinoids. Pharmacol Rev.
11 Horti A.G., Van Laere K. (2008). Development of radioligands for in vivo imaging of type 1 cannabinoid receptors (CB1) in human brain. Curr Pharm Des.
12 Akerman M.E., Pilch J., Peters D., Ruoslahti E. (2005). Angiostatic peptides use plasma fibronectin to home to angiogenic vasculature. Proc Natl Acad Sci U S A.
13 Gao M., Wang M., Miller K.D., Hutchins G.D., Zheng Q.H. (2010). Synthesis and in vitro biological evaluation of carbon-11-labeled quinoline derivatives as new candidate PET radioligands for cannabinoid CB2 receptor imaging. Bioorg Med Chem.
14 Fujinaga M., Kumata K., Yanamoto K., Kawamura K., Yamasaki T., Yui J., Hatori A., Ogawa M., Yoshida Y., Nengaki N., Maeda J., Zhang M.R. (2010). Radiosynthesis of novel carbon-11-labeled triaryl ligands for cannabinoid-type 2 receptor. Bioorg Med Chem Lett.
15 Evens N., Bormans G.M. (2010). Non-invasive imaging of the type 2 cannabinoid receptor, focus on positron emission tomography. Curr Top Med Chem.
16 Evens N., Muccioli G.G., Houbrechts N., Lambert D.M., Verbruggen A.M., Van Laere K., Bormans G.M. (2009). Synthesis and biological evaluation of carbon-11- and fluorine-18-labeled 2-oxoquinoline derivatives for type 2 cannabinoid receptor positron emission tomography imaging. Nucl Med Biol.
17 Evens N., Bosier B., Lavey B.J., Kozlowski J.A., Vermaelen P., Baudemprez L., Busson R., Lambert D.M., Van Laere K., Verbruggen A.M., Bormans G.M. (2008). Labelling and biological evaluation of [(11)C]methoxy-Sch225336: a radioligand for the cannabinoid-type 2 receptor. Nucl Med Biol.
18 Horti A.G., Gao Y., Ravert H.T., Finley P., Valentine H., Wong D.F., Endres C.J., Savonenko A.V., Dannals R.F. (2010). Synthesis and biodistribution of [11C]A-836339, a new potential radioligand for PET imaging of cannabinoid type 2 receptors (CB2). Bioorg Med Chem.
19 Yao B.B., Hsieh G., Daza A.V., Fan Y., Grayson G.K., Garrison T.R., El Kouhen O., Hooker B.A., Pai M., Wensink E.J., Salyers A.K., Chandran P., Zhu C.Z., Zhong C., Ryther K., Gallagher M.E., Chin C.L., Tovcimak A.E., Hradil V.P., Fox G.B., Dart M.J., Honore P., Meyer M.D. (2009). Characterization of a cannabinoid CB2 receptor-selective agonist, A-836339 [2,2,3,3-tetramethyl-cyclopropanecarboxylic acid [3-(2-methoxy-ethyl)-4,5-dimethyl-3H-thiazol-(2Z)-ylidene]-amide], using in vitro pharmacological assays, in vivo pain models, and pharmacological magnetic resonance imaging. J Pharmacol Exp Ther.